# Tricarbonyl[^99m^Tc]technetium(I)-((S)-6-(8-(bis(pyridin-2-ylmethyl)amino)octanamido)-2-((S)-1-carboxy-3-phenylpropylamino)hexanoyl)pyrrolidine-2-carboxylic acid

Chemical name: | Tricarbonyl[^99m^Tc]technetium(I)-((S)-6-(8-(bis(pyridin-2-ylmethyl)amino)octanamido)-2-((S)-1-carboxy-3-phenylpropylamino)hexanoyl)pyrrolidine-2-carboxylic acid
Abbreviated name: | ^99m^Tc-(CO)_3_D(C_8_)lisinopril
Synonym:
Agent Category: | Compound
Target: | Angiotensin-converting enzyme (ACE)
Target Category: | Enzyme-inhibitor binding
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of Signal/Contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure of ^99m^Tc-(CO)_3_D(C_8_)lisinopril

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=lisinopril)]

The renin–angiotensin system (RAS) plays a very important role in the regulation of blood pressure in humans (1-4). Renin is an enzyme produced in the kidneys, and it cleaves circulating angiotensinogen (a protein produced in the liver) to yield angiotensin I, an inactive decapeptide. The angiotensin-converting enzyme (ACE), found primarily in the lung, converts angiotensin I to angiotensin II, an active vasoconstrictor octapeptide. Angiotensin II also stimulates the production of aldosterone from the adrenal glands, which promotes retention of sodium and water. ACE is also responsible for inactivating bradykinin, a vasodilator (5). RAS and angiotensin II also play a role in interstitial fibrosis, cardiac remodeling and fibrosis, and heart failure (6, 7). It has been shown that RAS operates in the heart, and an upregulation of this system is correlated to heart failure (8-10). Inhibition of ACE in patients with heart failure has often resulted in a favorable outcome for the patient (11), although individuals treated with ACE inhibitors have been reported to respond differently as a result of genetic variations in the enzyme; a meta-analysis of data obtained from children of different races who had been treated with these inhibitors has shown the children reacted differently to the treatment (12, 13). In addition, the proper timing, optimal dosing, and monitoring of ACE inhibitor therapy for the individualized treatment of patients has not been fully worked out. Also, ACE appears to have a role in several other pathological conditions including myeloid leukemia, atherosclerosis, and diabetes (in the kidneys of patients) because an increased level of either the protein or its mRNA has been reported under these conditions (14-16).

In a preliminary radioautographic study, Dilsizian et al. showed that ACE expression correlated with the extent of the disease in patients with congestive heart failure and suggested that monitoring ACE expression may help monitor molecular remodeling of the heart (3). On the basis of this observation, Femia et al. envisioned that a radiotracer designed for imaging the RAS would be helpful for the development of individualized ACE inhibitor therapy (17). In this regard, a compound with high affinity for ACE, such as lisinopril or its derivative, would be best suited to study the expression of a radiotracer. Several derivatives of lisinopril that can incorporate rhodium or palladium while maintaining high affinity for ACE were reported and could probably be used to synthesize radiolabeled analogs of the compound (18). Using a single amino acid chelator technology based on the di(pyridylmethyl)amine chelator, Femia et al. synthesized a technetium-carbonyl (Tc(CO)_3_) core derivative of lisinopril and evaluated for the in vivo imaging of ACE expression in rats (17).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+lisinopril)]

Several lisinopril derivatives were synthesized as described by Femia et al. (17). Various, commercially available, ε-amino acids were converted to their di(pyridylmethylamino)alkanoic (D) acids through reductive amination using standard procedures (19). The ε-amino acid derivatives were converted to their lisinopril analogs as detailed by Femia et al. (17). The final products respectively contained 3 to 7 methylene units in the alkyl chain to form the D(C_4_)lisinopril, D(C_5_)lisinopril, or D(C_8_)lisinopril compounds. The various lisinopril derivatives (D(C_X_)L) had yields from 34% to 40% of the starting materials and were respectively characterized using nuclear magnetic resonance and by electrospray mass spectroscopy (17).

^99m^Tc-(CO)_3_D(C_8_)lisinopril was prepared with ^99m^Tc-(CO)_3_(H_2_O)_3_ using a commercially available kit as described by Femia et al. (17). Sodium [^99m^Tc]pertechnetate in saline was added to the radiolabeling kit, and the vial was heated in an oil bath at 100°C for 45 min. The reaction was stopped by the addition of 1 N HCl, and the product was added to another vial containing D(C_8_)lisinopril in methanol. The mixture was heated at 80°C for 1 h, and the product was purified on a C18 Sep-Pak plus cartridge activated with ethanol and washed with water. The loaded column was washed with water to remove all unreacted ^99m^Tc (which could include Tc(CO)_3_^+^ and TcO_4_^-^). The labeled compound was eluted from the cartridge with ethanol, and the solvent was removed under a stream of nitrogen. The radiochemical was subsequently reconstituted in 10% ethanol/saline. The radiochemical purity of the ^99m^Tc product was reported to be at least 98% with a yield of at least 88% as determined with high-performance liquid chromatography (HPLC). The specific activity of labeled lisinopril was reported to be 38,000 MBq/μm0l (1,027 mCi/μmol). The stability of the radiotracer was not reported (17).

Various non-radioactive rhenium (Re) complexes of D(C_x_)lisinopril were also synthesized to determine the in vitro activity of the compounds (17). For this, D(C_x_)lisinopril dissolved in methanol was mixed with [Re(CO)_3_(H_2_O)_3_]Br and heated at 80°C for 4 h. The solvent was then removed, and the product was purified with HPLC using a Dynamax C-18 reversed-phase column. The structure of the final product was determined with nuclear magnetic resonance and electrospray mass spectroscopy. The reaction yield of the Re-lisinopril complexes were not reported (17).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+lisinopril+in+vitro)]

The Re complexes of lisinopril containing the different methylene spacer units (C_4_, C_5_, or C_8_), as Re(CO)_3_D(C_x_)lisinopril, were evaluated in vitro against rabbit lung ACE (17). The activity of these compounds was reported to vary directly with the number of methylene spacers in the complex. The 50% inhibitory concentration (IC_50_) of Re(CO)_3_D(C_8_)lisinopril was 3 nM, followed by 144 nM for Re(CO)_3_D(C_5_)lisinopril and 1,146 nM for Re(CO)_3_D(C_4_)lisinopril. Similar IC_50_ values were obtained for the respective free D(C_x_)lisinopril compounds. The IC_50_ for the Re(CO)_3_D(C_8_)lisinopril analog was similar to the parent lisinopril (IC_50_ = 4 nM) compound (17).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

The biodistribution of ^99m^Tc-(CO)_3_D(C_8_)lisinopril was studied in Sprague-Dawley rats after an intravenous injection of the radiochemical (17). To demonstrate specificity of the radiotracer, some animals were injected with nonradioactive lisinopril 5 min before the administration of ^99m^Tc-(CO)_3_D(C_8_)lisinopril. The animals were euthanized by asphyxiation with carbon dioxide at 10, 30, 60, and 120 min after the injection (n = 5 animals per time point). Varying levels of the radiolabel were detected in the different tissue, and the levels decreased over time. The highest uptake was noticed in the lungs, which had 15.2% of the injected dose/g tissue (% ID/g) at 10 min and 3.39% ID/g remaining at 2 h; the lungs exhibit high ACE expression (17). Clearance of the radioactivity was mainly through the hepatobiliary route because an accumulation of the label in the intestine was reported to increase over time. Pretreatment of the animals with nonradioactive lisinopril before the administration of ^99m^Tc-(CO)_3_D(C_8_)lisinopril resulted in a markedly reduced (0.17% ID/g) accumulation of the label in the lungs, indicating that the label was highly specific for the targeted ACE (17).

Whole-body imaging was performed with ^99m^Tc-(CO)_3_D(C_8_)lisinopril in animals with or without pretreatment of nonradioactive lisinopril (n = 3 animals per group) (17). Images were obtained starting at 5 min after administration of the radioactivity for up to 60 min. The regions of interest were drawn over the lungs, liver, intestines, and the soft tissue (for background), and the regions of interest were quantified by counts after normalization to the background at the same time point. Quantitation of the radioactivity from the images reflected the same trends as obtained during the biodistribution study with uptake of the label primarily in the lungs and the intestines. Pretreatment of the animals with nonradioactive lisinopril was reported to block accumulation of radioactivity in the lungs.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+lisinopril+non+primate+mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+lisinopril+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Some studies reported in this chapter were supported by NIH, National Heart, Lung and Blood Institutes grant 1R43HL075918-01.

## References

1 Campbell D.J. (1987). Circulating and tissue angiotensin systems. J Clin Invest.
2 Chandrashekhar Y., Narula J. (2007). Exposing ACE up the sleeve. J Nucl Med.
3 Dilsizian V., Eckelman W.C., Loredo M.L., Jagoda E.M., Shirani J. (2007). Evidence for tissue angiotensin-converting enzyme in explanted hearts of ischemic cardiomyopathy using targeted radiotracer technique. J Nucl Med.
4 Ondetti M.A., Cushman D.W. (1981). Inhibition of the renin-angiotensin system. A new approach to the therapy of hypertension. J Med Chem.
5 Kuoppala A., Lindstedt K.A., Saarinen J., Kovanen P.T., Kokkonen J.O. (2000). Inactivation of bradykinin by angiotensin-converting enzyme and by carboxypeptidase N in human plasma. Am J Physiol Heart Circ Physiol.
6 Hirsch A.T., Talsness C.E., Schunkert H., Paul M., Dzau V.J. (1991). Tissue-specific activation of cardiac angiotensin converting enzyme in experimental heart failure. Circ res.
7 Bohm K., Kilter H., Kindermann M. (2003). Mechanisms contributing to the progression of left ventricular dysfunction to end-stage heart failure. Eur Heart J Suppl.
8 Paul M., Poyan Mehr A., Kreutz R. (2006). Physiology of local renin-angiotensin systems. Physiol Rev.
9 Shirani J., Narula J., Eckelman W.C., Dilsizian V. (2006). Novel imaging strategies for predicting remodeling and evolution of heart failure:targeting the renin-angiotensin system. Heart Failure Clin.
10 Shirani J., Dilsizian V. (2007). Molecular imaging of heart failure. Curr Opinion Biotechnol.
11 Brunner-La Rocca H.P., Vaddadi G., Esler M.D. (1999). Recent insight into congestive heart failure:focus on ACE inhibition and angiotensin-II antagonism. J Am Coll Cardiol.
12. Li, J., C. Baker-Smith, P. Smith, V. Hasselblad, M. Murphy, R. Califf, and D. Benjamin Jr, Racial Differences in Blood Pressure Response to Angiotensin-Converting Enzyme Inhibitors in Children: A Meta-Analysis. Clin Pharmacol Ther, 2008.
13 Yu H.M., Lin S.G., Liu G.Z., Zhang Y.Q., Ma W.J., Deng C.Y. (2006). Associations between CYP11B2 gene polymorphisms and the response to angiotensin-converting enzyme inhibitors. Clin Pharmacol Ther.
14 Beyazit Y., Aksu S., Haznedaroglu I.C., Kekilli M., Misirlioglu M., Tuncer S., Karakaya J., Koca E., Buyukasik Y., Sayinalp N., Goker H. (2007). Overexpression of the local bone marrow renin-angiotensin system in acute myeloid leukemia. J Natl Med Assoc.
15 Metzger R., Bohle R.M., Chumachenko P., Danilov S.M., Franke F.E. (2000). CD143 in the development of atherosclerosis. Atherosclerosis.
16 Konoshita T., Wakahara S., Mizuno S., Motomura M., Aoyama C., Makino Y., Kawai Y., Kato N., Koni I., Miyamori I., Mabuchi H. (2006). Tissue gene expression of renin-angiotensin system in human type 2 diabetic nephropathy. Diabetes Care.
17 Femia F.J., Maresca K.P., Hillier S.M., Zimmerman C.N., Joyal J.L., Barrett J.A., Aras O., Dilsizian V., Eckelman W.C., Babich J.W. (2008). Synthesis and evaluation of a series of 99mTc(CO)3+ lisinopril complexes for in vivo imaging of angiotensin-converting enzyme expression. J Nucl Med.
18 Pandurangi R.S., Katti K.V., Stillwell L., Barnes C.L. (1998). Retention of inhibitory potency of an ACE inhibitor conjugated with Rh(III) and Pd(II) (iminophosphorane)phosphines: synthesis and x-ray structure investigations. J Am Chem Soc.
19 Levadala M.K., Banerjee S.R., Maresca K.P., Babich J.W., Zubieta J.A. (2004). Direct reductive alkylation of amino acids: synthesis of bifunctional chelates for nuclear imaging. Synthesis.